# Cy7-Bis-dipicolylamine-zinc

Chemical name: | Cy7-Bis-dipicolylamine-zinc
Abbreviated name: | Cy7-DPA-Zn, Zn-DPA-Cy7
Synonym: | PSS-794, PSVue 794, Probe 1, Probe 2
Agent category: | Compound
Target: | Phosphatidylserine
Target category: | Phospholipid
Method of detection: | Optical near-infrared (NIR) fluorescence
Source of signal/contrast: | Cy7
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zn-DPA)]

Optical fluorescence imaging is increasingly being used to obtain images of biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in small animals.

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, atherosclerosis, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (3). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) (3) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V (or annexin A5) binding in necrosis because of disruption of the plasma membrane. Annexin V, a 36-kDa protein, binds to PS with high affinity (K_d_ = 7 nM). Annexin V has been radiolabeled with ^123^I ^124^I, and ^99m^Tc for imaging of cell death (4-6). Annexin V was successfully labeled with ^18^F (^18^F-labeled annexin V (4-[^18^F]FBA)) and is currently being developed as a positron emission tomography agent for imaging apoptosis as well as necrosis (7, 8). Cy5.5-Annexin V has been evaluated as an optical probe in small animals.

Gram-negative bacterium (e.g., Escherichia coli) and Gram-positive bacterium (e.g., Staphylococcus aureus) contain negatively charged molecules such as phosphatidylglycerol and phosphates in their cell membranes (9), whereas healthy mammalian cells primarily contain phospholipids of nearly neutral charge (10). Bis-dipicolylamine-zinc (DPA-Zn) showed selective affinity for anionic phospholipids (11, 12) on the surface of apoptotic bacteria and inflammatory neutrophils. Cy7, a NIR carbocyanine dye, was conjugated to DPA-Zn to form Cy7-DPA-Zn for in vivo NIR imaging of bacterial infection in mice (13, 14). Cy7-DPA-Zn was also able to detect apoptotic and necrotic cells (15-17).

### Related Resource Links:

- Chapters in MICAD (Annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Annexin%20V+AND+micad%5Bbook%5D), apoptosis (http://www.ncbi.nlm.nih.gov/books?term=apoptosis%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Annexin V (http://www.ncbi.nlm.nih.gov/gene/308))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Annexin V (http://www.ncbi.nlm.nih.gov/omim/131230))
- Clinical trials (Annexin V (http://www.clinicaltrials.gov/ct2/results?term=Annexin+V+))
- Drug information in FDA (Annexin V (http://google2.fda.gov/search?q=annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zn-DPA+synthesis)]

The synthesis of Cy7-DPA-Zn was described by Leevy et al. (14). Cy7 was conjugated to bis-dipicolylamine via a reaction with 4-hydroxybenzoic acid to form Cy7-bis-dipicolylamine (Cy7-DPA). Zinc nitrate was added to Cy7-DPA in ethanol. After 30 min of incubation, the solution was evaporated to provide Cy7-DPA-Zn. The extinction coefficient of Cy7-DPA-Zn is 110,000 cm^-1^M^-1^, and the quantum yield is 0.14. The absorption maximum of Cy7-DPA-Zn is 794 nm, and the emission maximum is 810 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zn-DPA+in+vitro)]

Leevy et al. (13) showed that incubation of Cy7-DPA-Zn with S. aureus in culture for 10 min effectively stained the periphery of the bacteria as observed with fluorescence microscopy. Leevy et al. (12) also showed that bacteria were clearly stained in preference to the membrane surface of human epithelial cells isolated from human saliva. Hanshaw et al. (11) showed that phosphatidylserine on the membrane surface of apoptotic cells (Jurkat, CHO, HeLa) were clearly stained in preference to the membrane surface of the counterpart healthy cells. Thakur et al. (18) showed that Cy7-DPA-Zn bound to apoptotic S. aureus and neutrophils and not to their normal counterparts with confocal microscopy.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zn-DPA+rodentia)]

Leevy et al. (13) performed in vivo fluorescence imaging in nude mice (n = 4) with an in vivo leg infection model in which 5 × 10^7^S. aureus colony-forming units were injected intramuscularly into the muscles overlaying the tibia bone. Cy7-DPA-Zn (0.075 mmol) was injected intravenously at 6 h after infection. The target/muscle ratio was 4.0 at 3 h and decreased slightly to 3.9 at 21 h. On the other hand, the target/liver ratio was 1.5 at 3 h and gradually increased to 2.7 at 21 h. Ex vivo imaging showed that the infected leg exhibited four-fold greater intensity than the liver and kidneys. Histoimmunochemical studies of frozen tissue sections confirmed the colocalization of Cy7-DPA-Zn with S. aureus in the infected leg. In another study, Thakur et al. (18) showed that the bacteria infection foci exhibited one-fold greater intensity than those in inflammation (turpentine-induced). No blocking experiment was performed.

Smith et al. (15) performed in vivo NIR fluorescence imaging studies of Cy7-DPA-Zn (3 mg/kg) in rats (n = 3) bearing rat PAIII prostate tumors. Whole-body images were obtained at every 3 h for 24 h after intravenous injection. The tumor was clearly visualized at 6 h after injection with tumor/non-tumor ratio of 2.5, which decreased to 2.2 at 24 h. The tumor/non-tumor ratios were 1.2 with injection of Cy7 at the time points studied. Ex vivo imaging at 24 h after injection confirmed the high tumor fluorescence intensity of Cy7-DPA-Zn with ~35-fold higher than Cy7. The highest fluorescence intensities were observed in the core of the tumor sections. The fluorescence intensity levels of Cy7-DPA-Zn in the liver, kidney and lung were ~50% lower than that of the tumor, whereas Cy7 exhibited little accumulation in the normal organs. Microscopic analysis showed that the fluorescence signal from Cy7-DPA-Zn colocalized with tumor’s necrotic regions. Smith et al. also performed various in vivo NIR fluorescence imaging studies of cell death in the thymus, muscle, and PAIII tumors of rodents treated with dexamethasone, chemicals (ionophore, ethanol, and ketamine), and radiation (16, 17), respectively. Cy7-DPA-Zn exhibited higher fluorescence intensities as compared with untreated controls. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zn-DPA+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zn-DPA+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zn-DPA+human)]

No publication is currently available.

## NIH Support

R01 GM059078, T32 GM075762, P50 CA94056, R01 GM36262

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
4 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
5 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
6 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
7 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
8 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
9 Matsumoto K. (2001). Dispensable nature of phosphatidylglycerol in Escherichia coli: dual roles of anionic phospholipids. Mol Microbiol.
10 Boon J.M., Smith B.D. (2002). Chemical control of phospholipid distribution across bilayer membranes. Med Res Rev.
11 Hanshaw R.G., Lakshmi C., Lambert T.N., Johnson J.R., Smith B.D. (2005). Fluorescent detection of apoptotic cells by using zinc coordination complexes with a selective affinity for membrane surfaces enriched with phosphatidylserine. Chembiochem.
12 Leevy W.M., Johnson J.R., Lakshmi C., Morris J., Marquez M., Smith B.D. (2006). Selective recognition of bacterial membranes by zinc(II)-coordination complexes. Chem Commun (Camb).
13 Leevy W.M., Gammon S.T., Johnson J.R., Lampkins A.J., Jiang H., Marquez M., Piwnica-Worms D., Suckow M.A., Smith B.D. (2008). Noninvasive optical imaging of staphylococcus aureus bacterial infection in living mice using a Bis-dipicolylamine-Zinc(II) affinity group conjugated to a near-infrared fluorophore. Bioconjug Chem.
14 Leevy W.M., Gammon S.T., Jiang H., Johnson J.R., Maxwell D.J., Jackson E.N., Marquez M., Piwnica-Worms D., Smith B.D. (2006). Optical imaging of bacterial infection in living mice using a fluorescent near-infrared molecular probe. J Am Chem Soc.
15 Smith B.A., Akers W.J., Leevy W.M., Lampkins A.J., Xiao S., Wolter W., Suckow M.A., Achilefu S., Smith B.D. (2010). Optical imaging of mammary and prostate tumors in living animals using a synthetic near infrared zinc(II)-dipicolylamine probe for anionic cell surfaces. J Am Chem Soc.
16 Smith B.A., Gammon S.T., Xiao S., Wang W., Chapman S., McDermott R., Suckow M.A., Johnson J.R., Piwnica-Worms D., Gokel G.W., Smith B.D., Leevy W.M. (2011). In vivo optical imaging of acute cell death using a near-infrared fluorescent zinc-dipicolylamine probe. Mol Pharm.
17 Smith B.A., Xiao S., Wolter W., Wheeler J., Suckow M.A., Smith B.D. (2011). In vivo targeting of cell death using a synthetic fluorescent molecular probe. Apoptosis.
18 Thakur, M.L., K. Zhang, B. Paudyal, D. Devakumar, M.Y. Covarrubias, C. Cheng, B.D. Gray, E. Wickstrom, and K.Y. Pak, Targeting Apoptosis for Optical Imaging of Infection. Mol Imaging Biol, 2011